# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-quantum dot-vascular endothelial growth factor

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-quantum dot-vascular endothelial growth factor
Abbreviated name: | ^64^Cu-DOTA-QD-VEGF, ^64^Cu-DOTA-QD-VEGF_121_
Synonym:
Agent Category: | Peptide
Target: | Vascular endothelial growth factor receptor 2 (VEGFR-2)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET), near-infrared (NIFR) optical imaging
Source of signal/contrast: | ^64^Cu, quantum dot (QD705)
Activation: | No
Studies: | - In vitro; - Rodents | No information is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu + QD +VEGF)]

Vascular endothelial growth factor (VEGF), also known as vascular permeability factor, is a homodimeric glycoprotein weighing ~45 kDa (1). The VEGF family consists of six groups: VEGF-A, -B, -C, -D, -E, and the placental growth factor (PIGF) (2). Structurally, VEGFs are related to the platelet-derived growth factors (PDGF), and they all contain the characteristic eight-cysteine residues known as the cysteine knot motif (3). Intrachain and interchain disulfide bonds are formed between these cysteine residues in conserved positions (2). VEGFs bind specifically to three cell-surface receptor tyrosine kinases, including fms-like tyrosine kinase-1 (Flt-1) or VEGF receptor-1 (VEGFR-1), kinase insert domain-containing receptor (KDR) or VEGRF-2, and Flt-4 or VEGFR-3. Each VEGFR contains a 750-amino acid-residue extracellular domain that is organized into seven immunoglobulin-like folds. VEGF and VEGFRs have been implicated in angiogenesis in many solid tumors, including breast cancer, colon cancer, hepatoma, bladder cancer, gastric cancer, and prostate cancer (3). VEGFR-2 (~220 kDa) is expressed exclusively in endothelial cells in cell differentiation, tumor vascularization, and metastasis. VEGF-A (the original VEGF) binds to the second and third extracellular immunoglobulin G loop of VEGFR-2 with a dissociation constant of ~100 pM (4). Hypoxia appears to be an important stimulus for producing VEGF in malignant and normal endothelial cells (3). Upon binding to its receptor VEGFR-2, VEGF-A elicits a pronounced angiogenic response, so it is considered as a predominant stimulator of angiogenesis. Human VEGF-A has five different isoforms generated by alternative slicing of a single pre-mRNA species, VEGF-A_121_, VEGF-A_145_, VEGF-A_165_, VEGF-A_189_, and VEGF-A_206_, which comprises 121,145,165, 189, and 206 amino acids, respectively (2). These isoforms differ in their ability to bind to heparin sulfate and extracellular matrix (ECM).

Quantum dots (QDs) are semiconductor nanocrystals of 2 to 10 nm in diameter (200–10,000 atoms) that possess a quantum confinement effect (hence the name “quantum dots”) caused by the restriction of electrons and holes in all three dimensions (5, 6). Like classic semiconductors that are composed of two types of atoms from the II/VI or III/V group elements in the periodic table, the nanocrystals have a valence band and a conduction band separated by an energy gap (band gap). Upon excitation, an electron is promoted from the filled valence band to the largely empty conduction band, which creates a positive vacancy “hole” in the valence band. The spatial separation (Bohr radius) of this electron-hole pair (“exciton”) is typically 1 to 10 nm for most semiconductors (6). The quantum confinement arises when one of the dimensions in the nanocrystals becomes comparable to its Bohr radius, these valence/conduction bands are quantized with an energy value that is directly related to the nanocrystal size. Thus, the excitons are confined in a manner similar to a particle-in-the-box problem, leading to a finite band gap and discretization of energy levels. When the electron fills the vacancy in the valence band, light of a certain wavelength is emitted, which corresponds to the respective band gap energy that is a function of nanocrystal size. For instance, the emission wavelength is 550 nm for 3-nm CdSe QDs and 650 nm for 7-nm CdSe QDs (7). The wavelength is also a function of semiconductor compositions, i.e., 5-nm CdTe has an emission wavelength of 700 nm, which is much higher than the 620 nm for 5-nm CdSe (8). QDs are 100 to 1,000 times more stable against photobleaching and are 10 to 100 times brighter than organic dyes. QDs have relatively long fluorescence lifetime (20–50 ns), which allows for time-resolved detection of their emitted fluorescence. For biological applications, QDs are generally encapsulated with biocompatible polymers that can increase their hydrodynamic diameter as much as two-fold (9). When their size is <5 nm, QDs are quickly cleared by renal filtration, whereas larger particles are more likely to be taken up by the reticuloendothelial system before reaching the targeted disease sites. Thus, after systematic administration, non-targeted QDs and some targeted QDs accumulate in substantial quantities in reticuloendothelial system, including the phagocytic cells in the liver, spleen, lymph nodes, and bone marrow (5). QDs can also accumulate in solid tumor tissue through the enhanced permeability and retention (EPR) effect regardless of whether they are conjugated with targeting ligands. As a whole, QDs have been widely used in cell trafficking, vasculature imaging, sentinel lymph node mapping, neural imaging, and targeting imaging (5).

^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-QD-VEGF factor (^64^Cu-DOTA-QD-VEGF) is a multimodal agent used for imaging VEGFRs with positron emission tomography (PET) and near-infrared (NIFR) optical imaging (10). ^64^Cu-DOTA-QD-VEGF consists of three components. An amine-functionalized QD (QD705) is used as a NIFR sensor and as a platform for carrying target-specific ligands. VEGF proteins are attached to the surface of QDs for recognition of VEGFRs. Complexes of the macrocyclic chelating agent DOTA with ^64^Cu(II) (^64^Cu-DOTA) are also covalently attached to the surface of QDs. ^64^Cu is a positron-emitting radionuclide with an intermediate half-life (12.7 h) that decays by positron (β^+^) with a branching factor of 17.4% and a maximum β^+^ energy of 0.653 MeV (11). ^64^Cu has been used as a radiotracer in PET imaging and as a radiotherapy agent in cancer treatment. QD705, which is commercially available, comprises a CdTe core shell with a thin layer of ZnS and polyethylene glycol (PEG2000)-attached amine groups (12). The emission wavelength of QD705 (705 nm) is located in the NIRF region (700–900 nm) where the absorbance of all biomolecules reaches a minimum (10). The use of a ZnS shell can increase the quantum yield of CdTe up to 30% to 50% (5). The PEG is used to decrease surface charge, increase colloidal stability of QDs, and reduce non-specific binding of QDs (13). Although QDs are used to examine cellular alteration, their in vivo detection is limited by the penetration depth of light. Thus, PET as a highly sensitive and quantitative modality can provide complementary information about tissues in depth. This PET/NIRF dual-modality probe may combine the advantages of QD optical imaging and PET imaging to assess the pharmacokinetics and targeting efficacy of QDs.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + QD +VEGF)+AND+synthesis%0D%0A)]

Chen et al. briefly described the synthesis of ^64^Cu-DOTA-QD-VEGF (10). Initially, DOTA was activated with 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide (EDC) and sulfo-N-hydroxy-sulfosuccinimide (SNHS) in a molar ratio of 10:5:4 (pH 5.5). The activated DOTA and 4-maleiidobutyric acid N-hydroxy-sulfosuccinimide (MAL-NHS) were added to the solution of QDs (QD705) in a molar ratio of 500:500:1 (pH 8.5) to produce DOTA-QD-MAL. VEGF_121_ was thiolated in situ by reaction with N-succinimidyl-S-acetylthioacetate (SATA), and then conjugated to DOTA-QD-MAL in a ratio of 10:1 (pH 7.0) to give DOTA-QD-VEGF. Complexation of DOTA-QD-VEGF with ^64^Cu(II) (pH 6.5) produced a >90% efficiency for ^64^Cu labeling. The radioactive specificity is 60 pmol QDs per mCi of ^64^Cu.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + QD +VEGF)+AND+%22in+vitro%22)]

Chen et al. examined the in vitro binding specificity of ^64^Cu-DOTA-QD-VEGF to VEGFR-2 (10). Porcine aortic endothelia (PAE/VEGFR-2) cells transfected with human VEGFR-2 were incubated with 1 nM DOTA-QD-VEGF in serum-free F12 Hams growth medium for 30 min and then examined with fluorescence microscope. The QD fluorescence overlaid well with the PAE/VEGFR-2 cells, suggesting a receptor-mediated internalization of the QD conjugate caused by a specific binding of DOTA-QD-VEGF to VEGFR-2. In comparison, no significant staining was observed for DOTA-QD-VEGF that was incubated with VEGFR-negative PAE cells. The binding affinity of DOTA-QD-VEGF was examined in PAE/VEGFR-2 cells in the presence of competitive ligand ^125^I-VEGF165. Similar to VEGF, the QD conjugate (DOTA-QD-VEGF) inhibited the binding of ^125^I-VEGF165 to VEGFR-2 in a dose-dependent manner. The 50% inhibition concentration was 4.1 nM for DOTA-QD-VEGF, which was very close to the 5.3 nM for VEGF, indicating that the QD conjugation caused no significant change in its VEGFR-2 binding affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + QD +VEGF) +AND++rodentia)]

The uptake of ^64^Cu-DOTA-QD-VEGF was first examined in tumor-bearing mice ex vivo with PET and NIRF imaging (10). Athymic mice were inoculated with U87MG (human glioblastoma) cells on the front flank. When the tumor grew to 200–500 mm^3^ (3–4 weeks), the mouse was intravenously injected with ^64^Cu-DOTA-QD-VEGF (20 pmol QD per 7–14 MBq ^64^Cu) and euthanized 4 h later. The major organs (liver, spleen, U87MG tumor, heart, lung, kidneys, bone, and muscle) were collected. Half of the tissue was quickly embedded for subsequent fluorescence microscopy. The other harvested tissue was used for microPET and NIRF imaging. For both imaging modalities, all major organs exhibited similar intensity patterns with a strong signal found in liver, spleen, and bone. The U87MG tumors demonstrated a higher uptake than the heart, kidney, and muscle. The QD fluorescence in the tumor tissue exhibited a non-homogeneous distribution. The U87MG tumor tissues were incubated with rat anti-mouse VEGFR-2 antibody and visualized with FITC-conjugated goat anti-rat antibody for immunofluorescence staining. The results demonstrated that DOTA-QD-VEGF was found co-localized with the VEGF/VEGFR-2 on the tumor vasculature with a small portion of extravasated QD conjugate.

The uptake of DOTA-QD-VEGF was then examined in the same in vivo tumor model with NIRF imaging (10). Athymic nude mice bearing subcutaneous U87MG tumors (5-8 nm in diameter) were injected intravenously with DOTA-QD-VEGF (200 pmol QD). Tumor fluorescence intensity increased over time and exhibited good contrast with respect to the background tissue. In comparison, no tumor contrast was observed in mice injected with DOTA-QD as a control. The non-specific uptake of both DOTA-QD and DPTA-QD-VEGF was apparent, as shown in the particularly bright fluorescence found in the bone marrow, spleen, and liver. The uptake of ^64^Cu-DOTA-QD-VEGF was further examined in the same in vivo tumor model with PET imaging (10). Athymic nude mice bearing subcutaneous U87MG tumors were injected intravenously with ^64^Cu-DOTA-QD-VEGF (20 pmol QD per 7–14 MBq ^64^Cu). PET images collected at multiple time points after injection demonstrated a prominent uptake of the QD conjugates in the liver, spleen, lymph node, and bone marrow. Comparing the PET images with the NIRF image, the signal in the tumors demonstrated a different pattern: the signal in NIRF decreased with time, whereas the signal in PET increased. This may reflect a receptor-mediated internalization of ^64^Cu-DOTA-QD-VEGF followed by degradation of the QD conjugate that led to some trapping of ^64^Cu inside the tumor. As a control, mice were injected with ^64^Cu-DOTA-QD. The uptake of ^64^Cu-DOTA-QD-VEGF in the mice with the U87MG tumors was much higher than in the mice injected with ^64^Cu-DOTA-QD. No significant differences were found in the mouse liver uptake, which were both ~50% injected dose (ID)/g of tissue. The tumor uptake of ^64^Cu-DOTA-QD-VEGF was 1.5 ± 0.6% ID/g, 2.8 ± 0.3% ID/g, 3.8 ± 0.6% ID/g, and 4.2 ± 0.5% ID/g at 1,4,16, and 24 h. The uptake of ^64^Cu-DOTA-QD was ≤1% ID/g.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + QD +VEGF) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + QD +VEGF) +AND+human)]

No publication is currently available.

### NIH Support

CA 119053, CA 121842, CA 102123, CA 114747, CA 119367, CA 93862

## References

1 Carmeliet P. (2005). VEGF as a key mediator of angiogenesis in cancer. Oncology.
2 Kiselyov A., Balakin K.V., Tkachenko S.E. (2007). VEGF/VEGFR signalling as a target for inhibiting angiogenesis. Expert Opin Investig Drugs.
3 McMahon G. (2000). VEGF receptor signaling in tumor angiogenesis. Oncologist.
4 Cross M.J., Dixelius J., Matsumoto T., Claesson-Welsh L. (2003). VEGF-receptor signal transduction. Trends Biochem Sci.
5 Zhang H., Yee D., Wang C. (2008). Quantum dots for cancer diagnosis and therapy: biological and clinical perspectives. Nanomed.
6 Sharma P., Brown S., Walter G., Santra S., Moudgil B. (2006). Nanoparticles for bioimaging. Adv Colloid Interface Sci.
7 Hild W.A., Breunig M., Goepferich A. (2008). Quantum dots - nano-sized probes for the exploration of cellular and intracellular targeting. Eur J Pharm Biopharm.
8. Smith, A.M., H. Duan, A.M. Mohs, and S. Nie, Bioconjugated quantum dots for in vivo molecular and cellular imaging. Adv Drug Deliv Rev, 2008.
9 Qi L., Gao X. (2008). Emerging application of quantum dots for drug delivery and therapy. Expert Opin Drug Deliv.
10. Chen, K., Z.B. Li, H. Wang, W. Cai, and X. Chen, Dual-modality optical and positron emission tomography imaging of vascular endothelial growth factor receptor on tumor vasculature using quantum dots. Eur J Nucl Med Mol Imaging, 2008.
11 McQuade P., Martin K.E., Castle T.C., Went M.J., Blower P.J., Welch M.J., Lewis J.S. (2005). Investigation into 64Cu-labeled Bis(selenosemicarbazone) and Bis(thiosemicarbazone) complexes as hypoxia imaging agents. Nucl Med Biol.
12 Cai W., Chen X. (2008). Preparation of peptide-conjugated quantum dots for tumor vasculature-targeted imaging. Nat Protoc.
13 Alivisatos A.P. (1996). Semiconductor clusters, nanocrystals, and quantum dots. Science.